# ^68^Ga-Labeled NODAGA-conjugated ghrelin receptor agonists and inverse agonists

Chemical name: | ^68^Ga-Labeled NODAGA-conjugated ghrelin receptor agonists and inverse agonists
Abbreviated name: | [^68^Ga]-NODAGA-ghrelin derivatives
Synonym:
Agent Category: | Peptides
Target: | Ghrelin receptor (growth hormone secretagogue receptor (GHS-R1a))
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin&cmd=DetailsSearch)]

Ghrelin is a 28-amino-acid peptide hormone that is produced and secreted mainly by the gastric mucosa and triggers the secretion of growth hormone (GH) from the pituitary by binding to the ghrelin receptor (previously known as the GH secretagogue receptor 1a or GHSR1a) (1). Although ghrelin is known to have several endocrine functions, investigators are interested in this molecule primarily because it is known to stimulate appetite, promote energy storage, and play a role in the development of obesity (1, 2). Therefore, the ghrelin/GHSR pathway is considered to be an important target for the treatment of obesity, cachexia, and anorexia (2, 3). However, ghrelin has a low stability while in circulation, and there is a lack of information regarding its in vivo behavior and biodistribution (2). In order to gain insight into the biological behavior of the ghrelin receptor, radiolabeled peptide agonists and inverse agonists (an inverse agonist binds to the same receptor as an agonist but produces an effect that is opposite to that of the agonist)) were designed and evaluated by Chollet et al. for use with positron emission tomography (PET) (2). The ghrelin agonists and inverse agonists were conjugated to 1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid (NODAGA), a bifunctional chelating agent, and labeled with ^68^Ga ([^68^Ga]-ghrelin conjugates designated 1f-4f and 5e). The functional behavior of the tracers was investigated in vitro and the biodistribution and imaging properties of the labeled peptides was studied in rodents (2).

### Related Resource Links

Ghrelin (http://omim.org/entry/605353) in Online Mendelian Inheritance in Man Database (OMIM)

Growth hormone secretagogue receptor (http://omim.org/entry/601898) (GHSR) in OMIM

Clinical trials with ghrelin (http://clinicaltrials.gov/ct2/results?term=Ghrelin+)

Clinical trials with ghrelin agonists (http://clinicaltrials.gov/ct2/results?term=Ghrelin+agonist)

Clinical trials with ghrelin antagonists (http://clinicaltrials.gov/ct2/results?term=Ghrelin+antagonist)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The various ghrelin peptide derivatives were synthesized on a multiple peptide synthesizer (for the designated name and amino acid sequence of each peptide, see Table 1), and each peptide was labeled with ^68^Ga as described by Chollet et al. (2). The radiochemical purity and specific activities of the labeled peptides are given in Table 1.

Table 1: Structure and nature of ghrelin derivatives ( 2 ).

Designated Number | Ghrelin Derivative* | Radiochemical Purity (%) | Specific Activity (GBq/μmol)
1e | N^α^-NODAGA[^68^Ga]-ghrelin(1–28) | - | -
2f (2e) ^ a ^ | [K^16^(NODAGA[^68^Ga]]ghrelin(1–28) | 96.7 ± 4.0 | 23.4 ± 6.6 (631.8 ± 178.2)^b^
3f (3e) | [Dpr^3^;K^16^(NODAGA[^68^Ga])]ghrelin(1–28) | 99.5 ± 0.5 | 12.6 ± 1.1 (340.2 ± 29.7)
4f (4e) | [Dpr^3^;K^16^(NODAGA[^68^Ga])]ghrelin(1–16) | 95.8 ± 4.5 | 8.4 ± 6.2 (226.8 ± 167.4)
5e (5d) | N^α^-NODAGA[^68^Ga]-KwFwLL-CONH_2_ | 96.2 ± 4.3 | 16.1 ± 2.4 (434.7 ± 64.8)

*The amino acid sequence of ghrelin is NH_2_-GSS^3^FLSPEHQRVQQRKESKKPPAKLQPR-COOH. The presence of an n-octanoyl group (C8:0) on Ser^3^ is essential for the biological activity of ghrelin (4).

a: Designated name of peptide containing nonradioactive Ga.

b: Specific activity in mCi/μmol.

The radiochemical yields of the different labeled peptides were not reported. The final preparation of each ^68^Ga-labeled compound was formulated in electrolyte solution E-153 (for composition, see Chollet et al. (2)) for storage.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin%20agonists%20and%20inverse%20agonists%20AND%20in%20vitro&cmd=DetailsSearch)]

The biological activity of nonradioactive ghrelin derivatives (1e-4e and 5d) was investigated with an inositol phosphate assay using African green monkey kidney COS-7 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1651&Template=cellBiology) cells (2). The EC_50_ values of the different peptides are presented in Table 2. Peptides 1e (with NODAGA(Ga) on the N-terminus), 3e, and 4e (both with NODAGA(Ga) at Lys^16^) showed a >1,800-, 3.5-, and 2.6-fold weaker activity compared with ghrelin, respectively. The 5d peptide had a >1,000-fold higher EC_50_ compared with ghrelin. Only peptide 2e (with NODAGA(Ga) at Lys^16^) had activity comparable to that of ghrelin. Peptides 1e-4e were reported to show an agonist behavior at the ghrelin receptor, and only 5d behaved as an inverse agonist (Table 2). On the basis of these results, only ^68^Ga-labeled 2f-4f and 5e were used for the in vivo studies.

Table 2: In vitro activity of nonradioactive ghrelin derivatives in an inositol phosphate turnover assay ( 2 ).

Peptide | EC _ 50 _ (nM) | Fold EC _ 50 _ over that of ghrelin | Nature (A or IA) ^ a ^
Ghrelin | 0.55 ± 0.241 | 1 | A
1e | >1,000 | >1,800 | A
2e | 0.72 ± 0.061 | 1.3 | A
3e | 1.91 ± 0.403 | 3.5 | A
4e | 1.41 ± 0.602 | 2.6 | A
5d | 643 ± 9.1 | >1,000 | IA

a: A = agonist; IA = inverse agonist.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin%20agonists%20and%20inverse%20agonists%20AND%20rodentia&cmd=DetailsSearch)]

For biodistribution studies, male Wistar rats (n = 4 animals/time point) were injected with 0.3 MBq (8.1 μCi) of each ^68^Ga-labeled peptide (2f-4f and 5d) through the tail vein, and the rodents were euthanized at 5 min and 60 min postinjection (p.i.) (2). All the major organs and blood were harvested from the animals to determine the amount of radioactivity accumulated in the different tissues. The amount of tracer present in each organ was expressed as a percent of injected dose per gram tissue (% ID/g). At 5 min p.i., the label was present mainly in the kidney with 2f, 3f, and 4f and with accumulation values of 26.6 ± 11.8% ID/g, 33.2 ± 2.2% ID/g, and 27.7 ± 2.9% ID/g, respectively. By 60 min p.i. the amount of tracer in the kidney from these radiochemicals increased to 63.3 ± 25.9% ID/g, 65.3 ± 2.2% ID/g, and 52.3 ± 5.9% ID/g, respectively. The amount of label in the liver with 2f, 3f, and 4f at 60 min p.i. was 8.1 ± 0.8% ID/g, 22.3 ± 2.4% ID/g, and 3.4 ± 0.2% ID/g, respectively. In the intestine, the amount of radioactivity from these tracers at 60 min p.i. was 0.9 ± 0.1% ID/g, 1.5 ± 0.4% ID/g, and 10.7 ± 2.1% ID/g, respectively. All other organs showed an accumulation of <1.0% ID/g at both time points. From these observations the investigators concluded that all the agonist tracers (2f-4f) were eliminated mainly through the urinary and the hepatobiliary system of the animals.

No change in accumulation of radioactivity in the kidney was observed with 5e (inverse agonist) at both time points (4.4 ± 0.2% ID/g and 4.4 ± 0.6% ID/g at 5 min p.i. and 60 min p.i., respectively). However, the accumulation of label from this tracer in the liver was 11.6 ± 1.4% ID/g and and 9.1 ± 2.0% ID/g at 5 min p.i. and 60 min p.i. , respectively. In the intestine the uptake was 9.4 ± 0.7% ID/g and 10.7 ± 2.1% ID/g at 5 min p.i. and 60 min p.i., respectively. . In addition, the concentration of radioactivity from 5e was higher in the blood at both time points (3.78 ± 0.43% ID/g and 1.53 ± 0.25% ID/g at 5 min p.i. and 60 min p.i., respectively) compared with the agonist-labeled compounds (with all these radiolabeled compounds, the amount of radioactivity in the blood was <2.0% ID/g and <0.3% ID/g at 5 min p.i. and 60 min p.i., respectively). No blocking studies were reported so the extent of specific binding could not be determined.

To investigate the metabolic stability of 2f-4f and 5e, the labeled compounds were administered to the rats as before (number of animals not reported), and arterial blood and urine samples were taken from the animals at various time points ranging from 1 min p.i. to 60 min p.i (2). Plasma separated from the whole blood was subjected to radio-high-performance liquid chromatography analysis with a Zorbax C_18_ 300SB column. Among all the radiolabeled ghrelin derivatives, only the inverse agonist 5e was reported to remain stable under in vivo conditions. With this tracer, <5% of the total radioactivity was associated with metabolites in the blood at 60 min p.i., and in urine the label was detected in trace amounts of the metabolites at this time point. In contrast, all the agonists had 40% (2f and 3f) to 100% (4f) of their label associated with at least two metabolites in the blood and the urine at this time point.

For PET imaging, 90 ± 33 MBq (2.4 ± 0.81 mCi) ^68^Ga-labeled 2f-4f and 5e was infused over 1 min into the tail vein of anesthetized, spontaneously breathing rats (n = 4 animals/time point) (2). With 2f and 4f the radioactivity was detected primarily in the kidney at 5 min p.i., and with 3f the label was observed mainly in the liver and the intestines. However, with 5e the tracer was visible in all the organs with higher concentrations in the kidney, liver, and the intestine. From time-activity curves it was apparent that the accumulation of radioactivity in the kidneys was rapid with 2f and 4f, intermediate for 3f, and slow with 5d. The curves showed that with 3f there was a high accumulation of label in the liver, and there was little change in accumulated radioactivity in the organ for up to 50 min p.i. Rapid accumulation of radioactivity in the hepatic tissue was observed with 2f, 4f, and 5e by ~1.5 min p.i., and the label was gradually lost from this organ by 50 min p.i. Rapid accumulation of label in the heart was observed with all the tracers at ~1.5 min p.i., followed by a rapid loss of radioactivity with the agonists. However, with 5e the loss of label from this organ was gradual but less pronounced.

From these studies based on the in vivo stability of the radiolabeled agonists and the inverse agonist, the investigators concluded that only 5e, the inverse agonist, appeared to be most suitable for the development of a peptide-based therapeutic for the treatment of obesity (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin%20agonists%20and%20inverse%20agonists%20AND%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin%20agonists%20and%20inverse%20agonists%20AND%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ghrelin%20agonists%20and%20inverse%20agonists%20AND%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lim C.T., Kola B., Korbonits M. (2011). The ghrelin/GOAT/GHS-R system and energy metabolism. Rev Endocr Metab Disord.
2 Chollet C., Bergmann R., Pietzsch J., Beck-Sickinger A.G. (2012). Design, evaluation, and comparison of ghrelin receptor agonists and inverse agonists as suitable radiotracers for PET imaging. Bioconjug Chem.
3 Soares J.B., Roncon-Albuquerque R., Leite-Moreira A. (2008). Ghrelin and ghrelin receptor inhibitors: agents in the treatment of obesity. Expert Opin Ther Targets.
4 Kojima M., Kangawa K. (2005). Ghrelin: structure and function. Physiol Rev.